# United States Food and Drug Administration (FDA) Warnings

## FDA warnings to the product labeling for the following contrast agents:

Gadolinium based contrast agents - The FDA has requested manufacturers of all gadolinium based contrast agents to add new warnings about exposure to gadolinium based contrast agents, which increases the risk for nephrogenic systemic fibrosis in patients with advanced kidney disease. The full text of the warning is available at: http://www.fda.gov/cder/drug/infopage/gcca/default.htm